# 3-(4-[^18^F]Fluorobenzyl)-8-methoxy-1,2,3,4 tetrahydrochromeno[3,4-c]pyridin-5-one

Chemical name: | 3-(4-[^18^F]Fluorobenzyl)-8-methoxy-1,2,3,4-tetrahydrochromeno[3,4-c]pyridin-5-one
Abbreviated name: | [^18^F]FMTP
Synonym:
Agent category: | Compound
Target: | Dopamine D_4_ receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FMTP%20and%20fluorine%20radioisotopes)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (1, 2). Dopamine receptors are involved in the pathophysiology of neuropsychiatric diseases, such as Parkinson’s disease, Alzheimer's disease, Huntington’s disease, and schizophrenia (3). Five subtypes of dopamine receptors, D_1_-_5_, were well-characterized pharmacologically and biochemically (4). These five subtypes were classified into two subfamilies of D_1_-like (D_1_, D_5_) and D_2_-like (D_2_, D_3_, D_4_) dopamine receptors. D_1_-like and D_2_-like receptors exert synergistic as well as opposite effects at the biochemical and overall system levels. A great majority of striatal D_1_ and D_2/3_ receptors are localized postsynaptically on the caudate-putamen neurons and to a lesser extent presynaptically on nigrostiatal axons. On the other hand, D_4_ receptors are mostly found in the extrastriatal regions of the brain, such as the cortex, hippocampus, thalamus and medulla. These areas are believed to control emotion and cognition.

Beside D_2_ receptors, D_4_ receptors may play an important role in the pathophysiology of schizophrenia from clinical studies of the atypical neuroleptic clozapine in patients (5, 6). Clozapine is not only effective against positive symptoms of schizophrenia but also is efficacious against the negative symptoms. Clozapine has a 10-fold greater affinity for D_4_ than for D_2_ receptors (7). However, it also has high affinities for 5-HT_1A,1B,2A,2C,6,7_, α_1A,2A,2C_, muscarinic M_1_ and histamine H_1_ receptors. The neurophysiologic role of D_4_ receptors remains to be defined. Thus, there is a need to for selective ligands to investigate the pharmacological role of D_4_ receptors.

There have been several attempts to develop specific D_4_ antagonists for PET radioligands for D_4_ receptors (8-10). However, none has proved suitable because of lack of selectivity and other pharmacological issues. Unangst et al. (11) reported that 3-(4-fluorobenzyl)-8-methoxy-1,2,3,4-tetrahydrochromeno[3,4-c]pyridin-5-one is a potent inhibitor of D_4_ receptors with >100-fold selectivity over D_2_ and D_3_ receptors. This led to the development of 3-(4-[^18^F]fluorobenzyl)-8-methoxy-1,2,3,4-tetrahydrochromeno[3,4-c]pyridin-5-one ([^18^F]FMTP) as a potential D_4_ receptor radioligand (12). [^18^F]FMTP was shown to identify extrastriatal D_4_ receptors in the regions of cortex and medulla in rat brain.

### Related Resource Links:

- Chapters in MICAD (Dopamine receptors (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=dopamine%20(receptors%20OR%20receptor)+%20AND+Table+AND+micad%5Bbook%5D))
- Gene information in NCBI (D_2_ receptor, (http://www.ncbi.nlm.nih.gov/gene/1813) D_3_ receptor (http://www.ncbi.nlm.nih.gov/gene/1814), D_4_ receptor (http://www.ncbi.nlm.nih.gov/gene/1815))
- Articles in Online Mendelian Inheritance in Man (OMIM) (D_2_ receptor (http://www.ncbi.nlm.nih.gov/omim/126450), D_3_ receptor (http://www.ncbi.nlm.nih.gov/omim/126451), D_4_ receptor (http://www.ncbi.nlm.nih.gov/omim/126452))
- Clinical trials (Dopamine receptors (http://www.clinicaltrials.gov/ct2/results?term=dopamine+receptor))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FMTP%5bAll%20Fields%5d%20AND%20synthesis%5bAll%20Fields%5d)]

4-[^18^F]Fluorobenzaldehyde was obtained by nucleophilic aromatic substitution of 4-trimethylammonium-benzaldehyde triflate with K[^18^F]F/Kryptofix2.2.2 in DMSO. [^18^F]FMTP radiosynthesis was accomplished by the reductive amination of 4-[^18^F]fluorobenzaldehyde with 8-methoxy-1,2,3,4-tetrahydrochromeno[3,4-c]pyridin-5-one, followed by high-performance liquid chromatography (HPLC) purification (12). The overall radiochemical yield of the radiosynthesis was 19.5% (decay corrected), the specific radioactivity was about 110 GBq/µmol (2.5 Ci/µmol) and the radiochemical purity was greater than 99%, the time of synthesis and purification was approximately 110 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FMTP%20AND%20in%20vitro)]

FMTP was reported to have high-affinity binding affinities to D_4_ receptor sites and not to D_2/3_ receptors in recombinant cell lines (11). The K_i_ values for D_2_, D_3_, and D_4_ receptors using [^3^H]spiperone were 5800, 548 and 4.3 nM, respectively. The D_2_/D_4_ K_i_ ratio was calculated to be 1,350.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FMTP%20AND%20rodentia)]

Biodistribution studies in rat showed a moderate accumulation of radioactivity in the whole brain, showing 0.6%, 0.5%, 0.4%, and 0.2% ID/g. at 2, 15, 30, and 120 min after injection of [^18^F]FMTP, respectively (12). There was a marked accumulation of the tracer in the frontal cortex within the first 10 min (0.69% ID/g), followed by a slow decrease of radioactivity to 0.35% ID/g at 60 min. The medulla exhibited a slightly higher radioactivity compared to other brain regions at 15, 30, 60 and 120 min. The maximum medulla-to-striatum and cortex-to-striatum ratios were 2.03 and 1.15, respectively. The accumulation of [^18^F]FMTP in frontal cortex and medulla were blocked by 1 mg/kg of unlabeled FMTP injected 15 min before the tracer with 84-86% decrease in radioactivity. The fraction of unchanged [^18^F]FMTP in blood samples determined by HPLC was 40% after 60 min after injection. The radioactivity remained intact in the brain. Further studies are needed to define the selectivity of [^18^F]FMTP as a D_4_ PET radioligand in vivo.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FMTP%20AND%20(dog%20or%20pig%20or%20rabbit%20ot%20sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FMTP%20AND%20(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20FMTP%20AND%20human)]

No publication is currently available.

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Seeman P., Bzowej N.H., Guan H.C., Bergeron C., Reynolds G.P., Bird E.D., Riederer P., Jellinger K., Tourtellotte W.W. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
4 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
5 Seeman P. (1992). Dopamine receptor sequences. Therapeutic levels of neuroleptics occupy D2 receptors, clozapine occupies D4. Neuropsychopharmacology.
6 Seeman P., Guan H.C., Van Tol H.H. (1993). Dopamine D4 receptors elevated in schizophrenia. Nature.
7 Van Tol H.H., Bunzow J.R., Guan H.C., Sunahara R.K., Seeman P., Niznik H.B., Civelli O. (1991). Cloning of the gene for a human dopamine D4 receptor with high affinity for the antipsychotic clozapine. Nature.
8 Bender D., Holschbach M., Stocklin G. (1994). Synthesis of n.c.a. carbon-11 labelled clozapine and its major metabolite clozapine-N-oxide and comparison of their biodistribution in mice. Nucl Med Biol.
9 Boy C., Klimke A., Holschbach M., Herzog H., Muhlensiepen H., Rota Kops E., Sonnenberg F., Gaebel W., Stocklin G., Markstein R., Muller-Gartner H.W. (1998). Imaging dopamine D4 receptors in the living primate brain: a positron emission tomography study using the novel D1/D4 antagonist [11C]SDZ GLC 756. Synapse.
10 Zhang M.R., Haradahira T., Maeda J., Okauchi T., Kawabe K., Noguchi J., Kida T., Suzuki K., Suhara T. (2002). Syntheses and pharmacological evaluation of two potent antagonists for dopamine D4 receptors: [11C]YM-50001 and N-[2-[4-(4-Chlorophenyl)-piperizin-1-yl]ethyl]-3-[11C]methoxybenzamide. Nucl Med Biol.
11 Unangst P.C., Capiris T., Connor D.T., Heffner T.G., MacKenzie R.G., Miller S.R., Pugsley T.A., Wise L.D. (1997). Chromeno[3,4-c]pyridin-5-ones: selective human dopamine D4 receptor antagonists as potential antipsychotic agents. J Med Chem.
12 Hai-Bin T., Duan-Zhi Y., Lan Z., Li-Hua W., Chun-Fu Z., Ming-Wei W., Chun-Ying W., Gu-Cai L., Yong-Xian W. (2005). Dopamine D(4) receptor antagonist 3-(4-[(18)F]fluorobenzyl)-8-methoxy-1,2,3,4-tetrahydrochromeno[3,4-c]pyrid in-5-one([(18)F]FMTP): radiosynthesis and in vivo characterization in rats. Appl Radiat Isot.